# Buried cyclo(Arg-Gly-Tyr(Me)-Lys-Glu) microbubbles

Chemical name: | Buried cyclo(Arg-Gly-Tyr(Me)-Lys-Glu) microbubbles
Abbreviated name: | bRGD-MBs
Synonym:
Agent category: | Peptide (nanoparticle)
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Ultrasound
Source of signal/contrast: | Microbubble
Activation: | Yes
Studies: | - In vitro | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=buried +RGD + microbubble)]

Microbubbles (MBs) are an aqueous suspension of a hydrophobic gas (perfluorocarbon or sulfur hexafluoride) encapsulated with stabilized shells of lipids, proteins, surfactants, or biocompatible polymers layer (1). The inherent material properties (density and compressibility) generate different speeds of sound in the gas core and the surrounding fluid (2). This leads to a mismatch in acoustic impedance on an order of 10,000, whereas the mismatch between different physiological tissues is around 1% (2). Ultrasound images are reconstructed from tissue-reflected echoes (backscatter) with an amplitude proportional to the impedance mismatch (3). The substantial mismatch between the echogenic MBs and the tissues allows for imaging vasculatures at high sensitivity (4). MBs that are 1–5 μm in diameter exhibit flow characteristics similar to erythrocytes in the blood stream (2). MBs can survive passage through the pulmonary vasculatures and the smallest capillaries (3), and they are removed from the circulation through filtration by the reticuloendothelial system and engulfment by the phagocytic cells (2). Because they are confined to the vascular system, MBs are designed to target the receptors expressed in diseased endothelial cells, including vascular endothelial growth factor receptor 2 (VEGFR2) and α_v_β_3_ integrins (angiogenesis), intracellular adhesion molecule 1 (ICAM1) (inflammation), and fibrinogen receptor GPIIb/IIIa (thrombosis) (5). These targeted MBs have various molecular probes attached on the shell surface, such as proteins, peptides, antibodies, and biotin-avidin complexes. Nevertheless, the presence of these probes may trigger immune activation and can lead to accelerated blood clearance (6). Thus, avoidance of an immunogenic response becomes important to the targeted MBs for minimizing hypersensitivity and enhancing accumulation at the target (7). A new architecture of the encapsulated shell has been developed for protecting recognition of ligands until they reach the target. This new architecture has utilized the ultrasound radiation force (USRF), also called Bjerknes force, produced from the interactions of the MBs with the ultrasound wave (7, 8).

Under ultrasound, MBs experience a large net radiation force in the direction of ultrasound wave propagation (8). The use of a cycling ultrasound pulse can deflect MBs over a distance of several millimeters as the result of the primary USRF, which concentrates the MBs near a vessel wall (8). At the same time, a secondary USRF that is present between individual MBs causes MBs to attract each other and accumulate along the vessel wall (8). Thus, the use of ultrasound pulse can facilitate the localization of targeted MBs along vessel walls, which has demonstrated a 20-fold improvement in the efficiency of MB adhesion (6). MBs with buried-ligand shell architecture (BLA) respond to the ultrasound differently compared to normal MBs (with the exposed ligand shell architecture (eRGD-MBs)) (9). BLA contain ligands that are tethered to the MB surface by polyethylene glycol (PEG) molecules and buried in a PEG overbrush (PEG with a much longer chain) (9). Without ultrasound, the buried ligands are concealed from blood components such as opsonins and phagocytes. The ultrasound-produced USRF can cause the forward movement of the MB mass center and the expansion of the encapsulated shell, which reveals the ligand to the target epitopes (7). This allows the targeting ligands to be hidden from the milieu until they reach the target site. Once they arrive at the target, the ultrasound pulse can be used to expose of the surface ligands and facilitate the adhesion of MBs. This protocol also reduces the nonspecific interactions between the ligands and the blood pool agents, maintains targeted agent viability, and reduces MB immunogenicity (9).

Buried cyclo(Arg-Gly-Tyr(Me)-Lys-Glu) MBs (bRGD-MBs) comprise a BLA type of ultrasound contrast agent that targets the α_v_β_3_ integrin receptors in endothelial cells (7). bRGD-MBs consist of perfluorobutane as the gas core, and distearoyl phosphatidylcholines (DSPC) and PEG conjugated distearoyl phosphatidylethanolamine (DSPE-PEG) as the encapsulated shell. The ligand RGD, which is the cell-recognition motif that is widely used to target the α_υ_β_3_ integrin (10), is covalently attached to the surface of the shell and buried in a PEG overbrush (PEG5k). The PEG5k is roughly three times thicker than the ligand-bearing inner layer and thus provides sufficient concealment for the ligands (9). This design can be extended to a variety of probes by adapting their surface characteristics to the microenvironment.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(buried + RGD + microbubble)+AND+synthesis%0D%0A)]

Borden et al. reported the detailed synthesis of bRGD-MBs (7). First, the construction of different shell architectures was initiated with mixing a variety of lipids in chloroform. bRGD-MBs contained 90 mol% DSPC, 2 mol% lipopolypeptide-cyclo(Arg-Gly-Tyr(Me)-Lys-Glu) (LPP-RGD), and 8 mol% DSPE-N-[methoxy(PEG)-5000] (DSPE-mPEG5000). The eRGD-MBs contained 90 mol% DSPC, 2 mol% LPP-RGD, and 8 mol% DSPE-N-[methoxy(PEG)-2000] (DSPE-mPEG2000). The control MBs contained 90 mol% DSPC and 10 mol% PEGylated species. These lipid solutions were dried and suspended in phosphate-buffered saline containing 1.0 mg lipid/ml as the precursor solution. Then the solution was exchanged with perfluorobutane and shaken in a mechanical device for 45 s to produce a milky, white suspension of microbubbles. The obtained microbubbles were diluted and washed three times with centrifugation flotation for 3 min at 300g. The size of these MBs was measured with an optical particle counter. The distribution of the size was centered at 1.8 μm diameter with secondary peaks at ~4.5 and ~7.5 μm diameter.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(buried +RGD + microbubble)+AND+%22in+vitro%22)]

Borden et al. studied the binding efficiency of bRGD-MBs in the presence of USFR in vitro (7). The cell adhesion integrin α_v_β_3_ expressed in human umbilical vein endothelial cells (HUVEC) was used to provide sites for binding RGD at high affinity. The lipophilic dye 1,1’-dioctadecyl-3,3,3’,3’-tetramethylindocarbocyanine perchlorate (DiI-C_18_(3)) was incorporated into the MB lipid shells for fluorescence detection. The MBs were raised by buoyancy to reach the HUVEC cells that adhered on the top of an acoustic chamber in 5 min. At this time point, the static experiment was conducted as the control; the acoustic experiment was performed by applying USRF pulse via a single piston transducer. The USRF pulse was composed of two sequential 5-s bursts with an ultrasound frequency of 2.5 MHz and a peak negative pressure (PNP) of 40 kPa. After application of the USRF pulse, the adhesion of MBs on the cells was imaged with epifluorescence and bright-field microscopy. The eRGD-MBs adhered to the cells to approximately the same extent through either buoyancy or USRF pulse. In contrast, the bRGD-MBs adhered to the cells at a density ~5.5-fold higher with the USRF pulse than with buoyancy. The adhered amount of bRGD-MBs under USRF was similar to that of the eRGD-MBs. In the static experiments, very few bRGD-MBs were observed to adhere to the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(buried +RGD + microbubble) +AND++rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(bruied +RGD + microbubble) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(bruied +RGD + microbubble) +AND+human)]

No publication is currently available.

### NIH Support

CA 097360, CA 103828

## References

1 Schneider M. (2008). Molecular imaging and ultrasound-assisted drug delivery. J Endourol.
2 Dayton P.A., Rychak J.J. (2007). Molecular ultrasound imaging using microbubble contrast agents. Front Biosci.
3 Hernot, S. and A.L. Klibanov, Microbubbles in ultrasound-triggered drug and gene delivery. Adv Drug Deliv Rev, 2008
4 Klibanov A.L. (2007). Ultrasound molecular imaging with targeted microbubble contrast agents. J Nucl Cardiol.
5 Sboros, V., Response of contrast agents to ultrasound. Adv Drug Deliv Rev, 2008
6 Lum A.F., Borden M.A., Dayton P.A., Kruse D.E., Simon S.I., Ferrara K.W. (2006). Ultrasound radiation force enables targeted deposition of model drug carriers loaded on microbubbles. J Control Release.
7 Borden M.A., Zhang H., Gillies R.J., Dayton P.A., Ferrara K.W. (2008). A stimulus-responsive contrast agent for ultrasound molecular imaging. Biomaterials.
8 Zhao S., Borden M., Bloch S.H., Kruse D., Ferrara K.W., Dayton P.A. (2004). Radiation-force assisted targeting facilitates ultrasonic molecular imaging. Mol Imaging.
9 Borden M.A., Sarantos M.R., Stieger S.M., Simon S.I., Ferrara K.W., Dayton P.A. (2006). Ultrasound radiation force modulates ligand availability on targeted contrast agents. Mol Imaging.
10 Ruoslahti E., Pierschbacher M.D. (1986). Arg-Gly-Asp: a versatile cell recognition signal. Cell.